# Radiolabeled (hetero)aromatic analogs of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and therapy of melanoma

Chemical name: | Radiolabeled (hetero)aromatic analogs of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and therapy of melanoma | [image]
Abbreviated name: | [^125^I]5a-I | [image]
Synonym: | [^125^I]5e, [^125^I]5h, [^125^I]5k, [^125^I]5l | [image]
Agent Category: | Compounds | [image]
Target: | Melanin | [image]
Target Category: | Others | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | | [image]
Studies: | - In vitro; - Rodents | Basic structure of radiolabeled compounds [^125^I]5a-I. Click on [^125^I]5e (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=24879192&loc=ec_rcs), [^125^I]5h (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=24879198&loc=ec_rcs), [^125^I]5k (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=44475984&loc=ec_rcs), and [^125^I]5l (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=24879251&loc=ec_rcs) for their structures in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=melanoma+and+imaging)]

Melanoma is one of the most deadly cancers in the United States. Although it accounts for only 4% of all skin cancer cases, melanoma is associated with ~79% of skin cancer–related deaths (1-4). The prognosis and the patient’s survival depend heavily on the clinical stage of the disease (http://www.cancer.gov/cancertopics/pdq/treatment/melanoma/HealthProfessional/page4) at the time of diagnosis. The 10-year survival rate for stage I melanoma patients is 90–97%, but only 3% for stage IV melanoma patients. Early detection and accurate assessment of the metastases remain the keys for improved outcome and disease-free survival. Unfortunately, the pattern of melanoma spread is often unpredictable, and conventional imaging with chest radiography, ultrasonography, computed tomography, and magnetic resonance imaging provides limited value for accurate staging and quantification of the disease burden (5, 6). Whole-body PET imaging with ^18^F-labeled fluorodeoxyglucose ([^18^F]FDG) has been shown to be superior to conventional imaging for detection of metastatic diseases, but it has not been shown to be useful for detecting small metastatic tumors (6, 7). Positive detection of nodal metastases requires nodal tumor involvement of more than 50% or capsular infiltration. Sub-centimeter pulmonary and hepatic metastases are frequently missed. Physiological uptake of FDG by the brain also limits its value in screening brain metastases. In an attempt to identify biomarkers of clinical utility, a large set of genes has been investigated for their abnormal expressions in melanoma (8-10). Potential biomarkers include p53, c-myc, CD44, Ki-67, Bcl-2, MITF, MMP2, p16, HIF2α, CXCR4, CEACAM1, p-Akt, β1 and β3 integrins, tPA, ICAM1, ephrin A1, β-catenin, P-cadherin, pleiotropin, PLK-1, and PUMA (8-10). Although these biomarkers offer the possibility of improved tumor staging through the molecular detection of microscopic metastases, these studies have been hampered by the failure of individual biomarkers to provide significant prognostic information beyond the current staging system.

Benzamide derivatives represent a versatile class of compounds used as agents for molecular imaging, as transporters for cytostatic agents, and as inhibitors for histone deacetylases (11). Since N-(2-diethylaminoethyl)-4-[^125^I]iodobenzamide ([^125^I]BZA) was first demonstrated to have high melanoma uptake, much effort has been made to further improve the affinity and pharmacological properties of this compound by modifying its structure, such as with the use of phenyl and amide substitutes (12-15). Most benzamide derivatives possess the common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1,2), and they exhibit comparable properties such as high melanoma uptake, which is a positive attribute for potentially useful imaging agents (11). The exact mechanism for the high melanoma uptake has not been fully established, although direct melanin binding, involvement in the melanin biosynthesis pathway, and sigma receptor mediation have been proposed as the most likely mechanisms for different derivatives. Chezal et al. synthesized a series of aromatic or heteroaromatic BZA analogs (1). These compounds were radioiodinated and designated as [^125^I]5a-I derivatives (from 5a to 5l). These derivatives incorporate the aromatic or heteroaromatic structures in place of the benzene moiety to take advantage of polycyclic aromatic compounds that display a strong affinity for melanin, while the lipophilic side chain was kept identical to the parent compound BZA. To facilitate the radiolabeling, iodine was preferably introduced on a benzene ring when possible. Analysis of the structure–activity relationships and the biological properties of the compounds in B16 melanoma-bearing mice showed that compounds 5e and 5I were superior to others as good candidates for scintigraphic imaging because of their rapid clearance from nontarget organs, while the compounds 5h and 5k were more favorable as agents for radionuclide therapy because of their high specific affinity for the tumor and the highest and longest lasting tumor uptake (1).

Benzamide Derivatives-Related Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Benzamide++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Chezal et al. described the synthesis and radiolabeling of each compound in detail (1). They incorporated the aromatic or heteroaromatic structures in place of the benzene moiety to take advantage of polycyclic aromatic compounds that display a strong affinity for melanin, while the lipophilic side chain was kept identical to the parent compound BZA. The radiochemical yields of the compounds varied from 22% to 92% (73%, 92%, 68%, and 69% for 5e, 5h, 5k, and 5I, respectively). The specific activities were 4.7–36.3 MBq/µmol (127–981 µCi/µmol) (7.1, 14.7, 11.7, and 15 MBq/µmol (192, 397, 316, and 405 µCi/µmol) for 5e, 5h, 5k, and 5I, respectively). The radiochemical purities of all compounds were >95%. The stability of the radiolabeled compounds was not evaluated.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Chezal et al. evaluated the in vitro binding of the compounds to melanin and their partition coefficients (1). Except for compound 5b (28.1%), all other analogs displayed a strong affinity (45−88%) for synthetic melanin in water. When melanin was suspended in phosphate-buffered solution (PBS), these values decreased strongly for compound 5f (from 75.3% to 11.6%) and were comparable to the values obtained with BZA, probably due to the ionic strength of PBS. For the other compounds, the binding to melanin was less affected in PBS, ranging from 35% to 59%. The lipophilicity values (log P) of the compounds appeared to some extent to be related to melanin binding affinity in water. However, the influence of PBS on the melanin binding differed between compounds, with no correlation to lipophilicity values. The percentages bound to melanin were 87.6%, 87.4%, 67.4%, and 44.8% in water and 56.1%, 43.2%, 47.3%, and 35.3% in PBS for 5e, 5h, 5k, and 5I, respectively. BZA was used here as a reference with 78.6% bound to melanin in water and 13.8% in PBS. The log P values were 1.54, 1.87, 1.12, and 0.51 for 5e, 5h, 5k, and 5I, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Biodistribution of the radioiodinated compounds was studied in C57BL6 male mice bearing the B16-F0 murine melanoma (n = 2 mice/compound) (1). In terms of the excretion, the compounds showed a broad panel of variations. Elimination was almost total after 72 h for most of the compounds (range, 90−100%), except for compound 5g, for which ~40% of the radioactivity remained in the mouse body at this time point. Compounds 5h, 5k, and BZA exhibited mainly urinary elimination, whereas 5c, 5d, 5g, and 5i mainly showed fecal excretion. Compounds 5e and 5f showed balanced distribution between the two routes. Concerning the tumor uptake, all of the ^125^I-labeled compounds demonstrated significant tumor uptake. The accumulation was observed from 1 h after injection (≥4.6% injected dose per gram tissue (ID/g)) and continued to be measurable at 72 h for all compounds. Compounds 5h, 5k, and 5l had the highest tumor uptake (≥17% ID/g) at 1 h after injection, while compounds 5h and 5k exhibited very long-lasting tumor concentrations (5.9 ± 1.7% ID/g for 5h and 12.5 ± 1.6% ID/g for 5k at 72 h after injection), 7-fold and 16-fold higher values, respectively, than BZA (0.8 ± 0.3% ID/g). Compounds 5h and 5k showed a kinetic profile favorable for application as a vector for radionuclide therapy. Compounds 5e, 5f, and 5l exhibited significant tumor uptake and very high specificity as illustrated by a rapid release from nontarget tissues, leading to high tumor to nontarget organ activity ratios. The tumor/liver, tumor/lung and tumor/ normal brain ratios at 1 h were 5.64, 3.38, and 15.4 for compound 5e, respectively, and 5.92, 9.86, and 27.14 for compound 5I, respectively. Because of the rapid release of the compounds from nontarget tissues, the tumor/nontarget organ activity ratios became very high and unquantifiable from 3 h after injection when organ concentration was within the range of the background value. The whole body biological half-life was 26.7 h for 5e, 30.2 h for 5l, 38.0 h for 5h, and 66.1 h for 5k. No blocking studies were reported.

Scintigraphic imaging was performed on one mouse after intravenous injection of compound 5k (1). The images illustrated the specific affinity for the tumor and a rapid clearance from nontarget organs, which allows well-defined imaging of the tumor until 72 h after administration. On the basis of these results, the authors concluded that compounds 5e and 5l, with their rapid clearance from nontarget organs, would be good candidates for scintigraphic imaging, allowing high-contrast images to be obtained promptly after administration. The quinoline compound 5h and the quinoxaline derivative 5k stood out due to their specific affinity for the tumor and the highest and longest lasting tumor uptake. They presented very favorable biological half-life values and dosimetry parameters for clinical application in radionuclide therapy of disseminated melanin containing melanoma; thus they appear to be very promising agents.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
2 Lens M. (2008). Current clinical overview of cutaneous melanoma. Br J Nurs.
3 Mohr P., Eggermont A.M., Hauschild A., Buzaid A. (2009). Staging of cutaneous melanoma. Ann Oncol.
4 McLoughlin J.M., Zager J.S., Sondak V.K., Berk L.B. (2008). Treatment options for limited or symptomatic metastatic melanoma. Cancer Control.
5 Choi E.A., Gershenwald J.E. (2007). Imaging studies in patients with melanoma. Surg Oncol Clin N Am.
6 Kochhar, R., H. Ali, S. Mak, and P. Manoharan, Metastatic cutaneous malignant melanoma: spectrum of imaging findings and the role of multimodality imaging. J Med Imaging Radiat Oncol, 200953(5): p. 467-78; quiz 478-9.
7 Essner R., Belhocine T., Scott A.M., Even-Sapir E. (2006). Novel imaging techniques in melanoma. Surg Oncol Clin N Am.
8 Gogas H., Eggermont A.M., Hauschild A., Hersey P., Mohr P., Schadendorf D., Spatz A., Dummer R. (2009). Biomarkers in melanoma. Ann Oncol.
9 Larson A.R., Konat E., Alani R.M. (2009). Melanoma biomarkers: current status and vision for the future. Nat Clin Pract Oncol.
10 Rother J., Jones D. (2009). Molecular markers of tumor progression in melanoma. Curr Genomics.
11 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
12 Michelot J.M., Moreau M.F., Labarre P.G., Madelmont J.C., Veyre A.J., Papon J.M., Parry D.F., Bonafous J.F., Boire J.Y., Desplanches G.G., et al. (1991). Synthesis and evaluation of new iodine-125 radiopharmaceuticals as potential tracers for malignant melanoma. J Nucl Med.
13 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
14 Garg, S., K. Kothari, S.R. Thopate, A.K. Doke, and P.K. Garg, Design, Synthesis, and Preliminary in Vitro and in Vivo Evaluation of N-(2-diethylaminoethyl)-4-[(18)F]fluorobenzamide ([(18)F]-DAFBA): A Novel Potential PET Probe to Image Melanoma Tumors. Bioconjug Chem, 2009
15 Ren G., Miao Z., Liu H., Jiang L., Limpa-Amara N., Mahmood A., Gambhir S.S., Cheng Z. (2009). Melanin-targeted preclinical PET imaging of melanoma metastasis. J Nucl Med.